# ^123^I-Anti-vascular cell adhesion molecule monoclonal antibody 5F10

Chemical name: | ^123^I-Anti-vascular cell adhesion molecule monoclonal antibody 5F10
Abbreviated name: | ^123^I-5F10
Synonym:
Agent Category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target Category: | Antibody-antigen binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+microbubble)]

Endothelial cells are important in inflammatory responses (1, 2). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (4-8). VCAM-1 binds to its counterligand, very late antigen-4 (VLA-4) integrin, on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (9). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. 5F10 is a murine monoclonal antibody (mAb) against rat VCAM-1 (10). ^123^I-Labeled 5F10 (^123^I-5F10) is being developed as a non-invasive tool for VCAM-1 expression in vascular endothelial cells in experimental colitis (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+attachment)]

The 5F10 mAb (1.67 nmol) was labeled with 15–25 MBq (0.41–0.68 mCi) [^123^I]NaI in the presence of tetrachlorodiphenylglycoluril (Iodogen) (11). ^123^I-5F10 was purified by gel filtration with <1% free ^123^I. No specific activity or radiochemical yield was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+rodentia)]

Sans et al. (11) performed biodistribution and scintigraphic studies of ^123^I-5F10 in control and colitic rats. In colitic rats, the organ with the highest mAb accumulation at 4 h after injection was the spleen (1,164.5 ng/g), followed by the colon (140 ± 30 ng/g), kidneys (96.5 ± 11.3 ng/g), ileum (48.8 ± 10.8 ng/g), and lungs (45.5 ± 4.0 ng/g). There were no differences between control and colitic rats in any of the extra-colonic organs studied. Only 20 ± 1 ng/g mAb accumulated in the colon of control rats. The accumulation of control antibody was significantly lower than control or colitic rats in all organ studies. Pretreatment with 5F10 decreased accumulation of ^125^I-5F10 by 80% in the colitic colon and by 40–75% in the other organs studied. Scintigraphic images were obtained in control and colitic rats at 2, 4, and 24 h after ^123^I-5F10 injection. The colon was clearly visible at 2–24 h in the colitic rats but not in the control rats. However, the liver and spleen were visible in both control and colitic rats. Pretreatment with 5F10 completely prevented the signal in the colon in the colitic rats at 2–24 h. The colon scintigraphic uptake correlated significantly (P < 0.01) with histological damage scores and with neutrophil infiltration.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+human)]

No publication is currently available.

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
5 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
6 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
7 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
8 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
9 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
10 Sans M., Panes J., Ardite E., Elizalde J.I., Arce Y., Elena M., Palacin A., Fernandez-Checa J.C., Anderson D.C., Lobb R., Pique J.M. (1999). VCAM-1 and ICAM-1 mediate leukocyte-endothelial cell adhesion in rat experimental colitis. Gastroenterology.
11 Sans M., Fuster D., Vazquez A., Setoain F.J., Piera C., Pique J.M., Panes J. (2001). 123Iodine-labelled anti-VCAM-1 antibody scintigraphy in the assessment of experimental colitis. Eur J Gastroenterol Hepatol.